# ^111^In/^68^Ga-Labeled DOTA conjugated cyclo[γ-D-Glu-Ala-Tyr-D-Lys]-Trp-Nle-Asp-Phe-NH_2_ (cyclo-MG2), a minigastrin analog

Chemical name: | ^111^In/^68^Ga-Labeled DOTA conjugated cyclo[γ-D-Glu-Ala-Tyr-D-Lys]-Trp-Nle-Asp-Phe-NH2 (cyclo-MG2), a minigastrin analog
Abbreviated name: | [^111^In/^68^Ga]-DOTA-cyclo-MG2
Synonym:
Agent Category: | Peptide
Target: | Cholecystokinin receptor subtype 2 (CCK2R)
Target Category: | Receptor
Method of detection: | Single photon emission computed tomography (SPECT) and gamma planar imaging for ^111^In; positron emission tomography (PET) for ^68^Ga
Source of signal / contrast: | ^111^In (SPECT); ^68^Ga (PET)
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=cck2%20receptor&cmd=DetailsSearch)]

The three subtypes of the cholecystokinin (CCK) receptors (CCKR) belong to the G-protein coupled receptor family and are classified (CCK1R, CCK2R and CCK2i4svR) on the basis of their affinities for the CCK and the gastrin peptides, differential distribution in the tissues and molecular structure (1). The CCK1R (previously known as CCKA) is found mainly on the peripheral cells of the pancreas and has a 500 to 1000-fold higher affinity for sulfated CCK compared with the non-sulfated ligand. In addition, the CCK1R is expressed mainly in organs of the gastrointestinal tract of rodents, but is expressed at low levels in humans (2). The CCK2R (previously known as CCKB) is expressed in the brain, stomach, pancreas and the gallbladder and exhibits an almost equivalent affinity for gastrin and sulfated or non-sulfated CCK (the CCK2R is also known as the gastrin receptor (GR)). Although CCK1R and CCK2R/GR are expressed in various normal tissues the CCK2R is overexpressed in most tumorous tissues such as medullary thyroid carcinomas (http://www.cancer.gov/cancertopics/pdq/genetics/medullarythyroid/HealthProfessional) (MTC; >90%), astrocytomas (http://www.cancer.gov/dictionary?cdrid=45602) (>65%) and stromal ovarian cancers (http://www.cancer.gov/cancertopics/types/ovarian) (100%). The CCK2i4svR is a splice variant of the CCK2R that is expressed only in colorectal and pancreatic neoplasms, but not in the normal colorectal mucosa (1). Several gastrin and CCK analogs that have a high affinity for the CCK2R have been developed and labeled with radionuclides for the detection and therapy of these cancers. It has been shown that radiolabeled CCK derivatives and mini gastrin (MG; a shorter version of human gastrin 1 that consists of amino acids 5-17 of the parent peptide) can be used with scintigraphy to detect colorectal or pancreatic cancer tumors that overexpress the CCK2i4svR (3) or to screen for patients who may benefit from the radiotherapy of this disease (4). In pre-clinical studies, however, these radiochemicals showed a high uptake of radioactivity in the kidneys thereby limiting their use in humans (5).

Two cyclized MG analogues, cyclo-MG1 (cyclo^1,9^[γ-D-Glu^1^,desGlu^2^−^6^,D-Lys^9^]MG) and cyclo-MG2 (cyclo^1,9^[γ-D-Glu^1^,desGlu^2^−^6^,D-Lys^9^,Nle^11^]MG) were synthesized, conjugated to metal chelating agents, labeled with ^99m^Tc and evaluated with single photon emission computed tomography (SPECT) for the detection of tumors that express the CCKR (6). The two ^99m^Tc-labeled cyclo-compounds were shown to be suitable to detect tumors, but they exhibited low in vitro stability and generated low quality scintigraphic images due to rapid degradation in vivo. Similar observations have been reported with other ^99m^Tc-labeled compounds that were used in a clinical trial for the visualization of tumors that overexpressed the CCK2R (7). In an ongoing effort to develop imaging agents that could be used to visualize tumors that express the CCK2R two 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (DOTA) conjugated cyclic MG analogs, cyclo[γ-D-Glu-Ala-Tyr-D-Lys]-Trp-Met-Asp-Phe-NH_2_ (DOTA-cyclo-MG1) and cyclo[γ-D-Glu-Ala-Tyr-D-Lys]-Trp-Nle-Asp-Phe-NH_2_ (DOTA-cyclo-MG2), were designed for labeling with either ^111^In (for SPECT imaging) or ^68^Ga (for imaging with positron emission tomography (PET)) (5). The biodistribution of the various radiolabeled compounds and their ability to detect xenograft tumors that express the CCK2R in mice was then investigated. This chapter presents the results obtained with ^111^In/^68^Ga- labeled DOTA-cyclo-MG2 ([^111^In/^68^Ga]-DOTA-cyclo-MG1). The biodistribution and imaging characteristics of ^111^In/^68^Ga- labeled DOTA-cyclo-MG1 are presented in a companion chapter in MICAD (www.micad.nih.gov) (8).

### Related Resource Links

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=CCKR+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Mouse cholecystokinin B receptor (CCK2R (http://www.ncbi.nlm.nih.gov/gene/12426)); NCBI-Gene ID: 12426

Mouse CCK2R nucleotide and protein (http://www.genome.jp/dbget-bin/www_bget?mmu:12426) sequences in Kyoto Encyclopedia of Genes and Genomes database (KEGG)

KEGG pathway (Mouse CCK2R (http://www.genome.jp/dbget-bin/get_linkdb?-t+pathway+mmu:12426))

Clinical trials (http://clinicaltrials.gov/ct2/results?term=cholecystokinin+receptor) related to cholecystokinin receptor

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-DOTA-cyclo-MG2%20synthesis&cmd=DetailsSearch)]

DOTA-cyclo-MG1 and DOTA-cyclo-MG2 was obtained from a commercial source and characterized with matrix-assisted laser desorption/ionization-time of flight mass spectrometry and reversed phase high-performance liquid chromatography (RP-HPLC) (5). The peptides were labeled with ^111^In or ^68^Ga as described by Guggenberg et al. (5). The specific activities of the labeled peptides were 2.7–4.1 MBq (72.9-110.7 μCi)/nmol and 5.3–13.6 MBq (143.1-367.2 μCi) /nmol with ^111^In and ^68^Ga, respectively and both the labeled peptides had radiochemical purities of >95% as determined with RP-HPLC. The radiochemical yields of the two radiolabeled peptides were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B111In%5D-DOTA-cyclo-MG2%20synthesis%20in%20vitro&cmd=DetailsSearch)]

Because ^68^Ga has a short half-life (~68 min) all the in vitro characterization studies were performed only with ^111^In-labeled DOTA-cyclo-MG1 and DOTA-cyclo-MG2 (half-life of ^111^In is ~2.8 d) (5). The in vitro stability of [^111^In]-DOTA-cyclo-MG1 and [^111^In]-DOTA-cyclo-MG2 was determined by incubating 500-1000 pmol of the labeled peptides for up to 24 h at 37^o^ C in phosphate buffered saline (PBS; pH not mentioned) and fresh human plasma, respectively. Although both the labeled peptide were >95% intact in PBS at 24 h after the incubation (as determined with RP-HPLC analysis) only 70% and 92.3% of [^111^In]-DOTA-cyclo-MG1 and [^111^In]-DOTA-cyclo-MG2, respectively, were unaltered in the plasma at the end of the incubation. In another study it was shown that at the end of incubation at 37^o^ C for 4 h with human plasma 20.4 ± 0.4% and 18.8 ± 2.0% of [^111^In]-DOTA-cyclo-MG1 and [^111^In]-DOTA-cyclo-MG2 were bound to the plasma proteins as determined with size-exclusion chromatography (5). Radio-HPLC analysis of [^111^In]-DOTA-cyclo-MG1 and [^111^In]-DOTA-cyclo-MG2 (each peptide was 500–1,000 pmol /mL) that had been respectively incubated with rat liver and kidney homogenates for 2 h at 37^o^ C revealed that both the labeled peptides were completely degraded within this time period (5).

Using an octanol/water mixture the partition coefficients (log P) of [^111^In]-DOTA-cyclo-MG1 and [^111^In]-DOTA-cyclo-MG2 were determined to be -3.08 ± 0.12 and -2.68 ± 0.10, respectively.

The receptor binding and cell uptake characteristics of [^111^In]-DOTA-cyclo-MG1 and [^111^In]-DOTA-cyclo-MG2 were studied with AR42J cells, a rat pancreatic cell line that expresses the CCK2R (5). Incubation of the labeled peptides with the cells for 2 h showed that 1.74 ± 0.07% and 0.93 ± 0.06% of the total added radioactivity was internalized by the cells with [^111^In]-DOTA-cyclo-MG1 and [^111^In]-DOTA-cyclo-MG2, respectively. From an autoradiographic assay with human MTC tissue sections and ^125^I-labeled CCK as the receptor ligand in presence of DOTA-cyclo-MG1 it was determined that the IC_50_ value of [^111^In]-DOTA-cyclo-MG1 for the receptor was 0.7 ± 0.12 nM (n = 3 determinations). The IC_50_ value of [^111^In]-DOTA-cyclo-MG2 was not reported. For comparison the IC_50_ value of CCK-8, a control linear peptide with a high affinity for the CCKR, was reported to be 0.06 ± 0.04 nM in the same assay.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B111In%5D-DOTA-cyclo-MG2%20synthesis%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^111^In/^68^Ga]-DOTA-cyclo-MG2 and [^111^In/^68^Ga]-DOTA-cyclo-MG1 was investigated in BALB/c nude mice bearing AR42J cell xenograft tumors on their right flank (5). The animals (n = 3 mice/time point/tracer) were injected through the tail vein with a mixture of 0.05 MBq (1.35 μCi) [^111^In]-DOTA-cyclo-MG2 and 1 MBq (27 μCi) [^68^Ga]-DOTA-cyclo-MG2 (this corresponded to <0.12 nmol total peptide). Two other groups of animals were injected with a similar mixture of [^111^In/^68^Ga]-DOTA-cyclo-MG1 (5). The mice were subsequently euthanized at 1 h and 4 h postinjection (p.i.) to determine the amount of radioactivity present in the various tissues. All results were expressed as percent of injected dose per gram tissue (% ID/g). Data in Table 1 and Table 2 shows that the pattern of radioactivity uptake from the ^111^In-labeled and ^68^Ga-labeled peptides, respectively, was similar within the groups of animals of each nuclide (5). In general, the accumulation of radioactivity in the various organs and the tumors was higher with the ^68^Ga-labeled peptides than with the ^111^In-peptides. However, the uptake of label from [^68^Ga]-DOTA-cyclo-MG2 (Table 1) in the different organs was higher than from [^68^Ga]-DOTA-cyclo-MG1 (Table 2). The tumor/muscle ratios with the labeled compounds were 4.19, 12.10, 10.56 and 11.54 with [^111^In]-DOTA-cyclo-MG2, [^68^Ga]-DOTA-cyclo-MG2, [^111^In]-DOTA-cyclo-MG1 and [^68^Ga]-DOTA-cyclo-MG1, respectively. In addition, radioactivity from the [^111^In]-labeled peptides was excreted primarily through the renal route, whereas radioactivity from the [^68^Ga]-labeled peptides was excreted mainly through the hepatobiliary route. To determine the receptor binding specificity of the labeled compounds the animals (n = 3 mice) were injected with a mixture of the two tracers ([^111^In/^68^Ga]-DOTA-cyclo-MG2 and [^111^In/^68^Ga]-DOTA-cyclo-MG1, respectively) along with approximately 30 nmol of non-radioactive human MG (5). The animals were euthanized at 1 h p.i. and all tissues of interest were retrieved from the mice as before. Under blocking conditions the tumors showed little change in the uptake of radioactivity with [^111^In/^68^Ga]-DOTA-cyclo-MG2 (Table 1), but with [^111^In/^68^Ga]-DOTA-cyclo-MG1 the uptake of radioactivity in the tumors was reduced by approximately 50% (Table 2) indicating that [^111^In/^68^Ga]-DOTA-cyclo-MG1 had a moderate binding specificity for CCK2R, but no such specificity was observed with [^111^In/^68^Ga]-DOTA-cyclo-MG2.

For SPECT imaging studies a mouse bearing AR42J cell tumors was injected with 10-15 MBq (27-40.5 μCi) of either [^111^In]-DOTA-cyclo-MG2 or [^111^In]-DOTA-cyclo-MG1 (~ 0.3 nmol peptide) as described above (5). Images acquired from the animal at 1 h p.i. showed that the tumor was clearly visible with [^111^In]-DOTA-cyclo-MG2 whereas in mice injected with [^111^In]-DOTA-cyclo-MG1 the lesion was visible only faintly at this time point. The tumor/kidney ratios calculated from the images were reported to be 0.92 and 0.01 for [^111^In]-DOTA-cyclo-MG2 and [^111^In]-DOTA-cyclo-MG1, respectively, and were different from those observed during the biodistribution study (see Table 1 and Table 2). No blocking studies were reported.

From these studies the investigators concluded that although [^111^In/^68^Ga]-DOTA-cyclo-MG2 and [^111^In/^68^Ga]-DOTA-cyclo-MG1 appear to be suitable for use as an imaging agent to visualize tumors that express the CCK2R, further studies are necessary to improve the targeting and pharmacokinetic properties of these MG analogues (5).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B111In%5D-DOTA-cyclo-MG2%20synthesis%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B111In%5D-DOTA-cyclo-MG2%20synthesis%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B111In%5D-DOTA-cyclo-MG2%20synthesis%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Laverman P., Sosabowski J.K., Boerman O.C., Oyen W.J. (2012). Radiolabelled peptides for oncological diagnosis. Eur J Nucl Med Mol Imaging.
2 Roosenburg S., Laverman P., van Delft F.L., Boerman O.C. (2011). Radiolabeled CCK/gastrin peptides for imaging and therapy of CCK2 receptor-expressing tumors. Amino Acids.
3 Laverman P., Roosenburg S., Gotthardt M., Park J., Oyen W.J., de Jong M., Hellmich M.R., Rutjes F.P., van Delft F.L., Boerman O.C. (2008). Targeting of a CCK(2) receptor splice variant with (111)In-labelled cholecystokinin-8 (CCK8) and (111)In-labelled minigastrin. Eur J Nucl Med Mol Imaging.
4 von Guggenberg E., Dietrich H., Skvortsova I., Gabriel M., Virgolini I.J., Decristoforo C. (2007). 99mTc-labelled HYNIC-minigastrin with reduced kidney uptake for targeting of CCK-2 receptor-positive tumours. Eur J Nucl Med Mol Imaging.
5 von Guggenberg E., Rangger C., Sosabowski J., Laverman P., Reubi J.C., Virgolini I.J., Decristoforo C. (2012). Preclinical Evaluation of Radiolabeled DOTA-Derivatized Cyclic Minigastrin Analogs for Targeting Cholecystokinin Receptor Expressing Malignancies. Mol Imaging Biol.
6 von Guggenberg E., Sallegger W., Helbok A., Ocak M., King R., Mather S.J., Decristoforo C. (2009). Cyclic minigastrin analogues for gastrin receptor scintigraphy with technetium-99m: preclinical evaluation. J Med Chem.
7 Kosowicz J., Mikolajczak R., Czepczynski R., Ziemnicka K., Gryczynska M., Sowinski J. (2007). Two peptide receptor ligands (99m)Tc-EDDA/HYNIC-Tyr(3)-octreotide and (99m)Tc-EDDA/HYNIC-(D)Glu-octagastrin for scintigraphy of medullary thyroid carcinoma. Cancer Biother Radiopharm.
8 Chopra, A., 111In/68Ga-Labeled DOTA conjugated cyclo[γ-D-Glu-Ala-Tyr-D-Lys]-Trp-Met-Asp-Phe-NH2 (cyclo-MG1), a minigastrin analog. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.

Table 1: Uptake of radioactivity (% ID/g) in various organs from [^111^In]-DOTA-cyclo-MG2 and [^68^Ga]-DOTA-cyclo-MG2

Tissue | [ ^ 111 ^ In]-DOTA-cyclo-MG2 | | | | [ ^ 68 ^ Ga]-DOTA-cyclo-MG2
Tissue | Time postinjection (p.i.)
Tissue | 1 h | 1 h Blocked | 4 h | Tumor/Tissue Ratio at 1 h | 1 h | 1 h Blocked | 4 h | Tumor/Tissue Ratio at 1 h
Blood | 0.50 ± 0.08 | 0.39 ± 0.11 | 0.07 ± 0.01 | 2.39 | 1.12 ± 0.25 | 0.63 ± 0.20 | 0.65 ± 0.34 | 3.68
Muscle | 0.23 ± 0.13 | 0.06 ± 0.02 | 0.05 ± 0.02 | 4.19 | 0.38 ± 0.19 | 0.09 ± 0.09 | 0.30 ± 0.08 | 12.10
Intestine | 0.92 ± 0.30 | 0.96 ± 0.12 | 0.80 ± 0.44 | 1.99 | 5.83 ± 1.50 | 6.37 ± 0.21 | 4.82 ± 1.25 | 0.69
Liver | 0.58 ± 0.09 | 1.07 ± 0.11 | 0.39 ± 0.03 | 1.90 | 5.59 ± 1.63 | 11.18 ± 1.83 | 5.70 ± 0.78 | 0.71
Kidney | 2.01 ± 0.20 | 2.39 ± 0.25 | 1.43 ± 0.03 | 0.60 | 1.57 ± 0.60 | 1.86 ± 0.29 | 1.01 ± 0.20 | 2.34
Tumor | 1.20 ± 0.24 | 1.10 ± 0.06 | 0.91 ± 0.19 | - | 3.51 ± 1.49 | 2.04 ± 0.30 | 3.56 ± 0.64 | -

For complete data, see von Guggenberg et al. ( 5 )

Table 2: Accumulation of radioactivity (% ID/g) in various organs from [^111^In]-DOTA-cyclo-MG1 and [^68^Ga]-DOTA-cyclo-MG1

Tissue | [ ^ 111 ^ In]-DOTA-cyclo-MG1 | | | | [ ^ 68 ^ Ga]-DOTA-cyclo-MG1
Tissue | Time postinjection (p.i.)
Tissue | 1 h | 1 h Blocked | 4 h | Tumor/Tissue Ratio at 1 h | 1 h | 1 h Bocked | 4 h | Tumor/Tissue Ratio at 1 h
Blood | 0.35 ± 0.01 | 0.20 ± 0.02 | 0.07 ± 0.06 | 3.11 | 1.21 ± 0.04 | 0.91 ± 0.12 | 0.53 ± 0.29 | 2.47
Muscle | 0.08 ± 0.02 | 0.03 ± 0.01 | 0.01 ± 0.00 | 10.56 | 0.25 ± 0.01 | 0.23 ± 0.02 | 0.22 ± 0.10 | 11.54
Intestine | 0.31 ± 0.05 | 0.28 ± 0.05 | 0.83 ± 0.77 | 3.63 | 3.84 ± 9.15 | 2.89 ± 0.23 | 3.19 ± 0.50 | 1.41
Liver | 0.28 ± 0.06 | 0.36 ± 0.06 | 0.21 ± 0.12 | 3.23 | 1.85 ± 0.37 | 2.75 ± 0.09 | 3.10 ± 0.76 | 0.77
Kidney | 2.10 ± 0.47 | 1.67 ± 0.30 | 1.84 ± 0.37 | 0.66 | 1.48 ± 0.31 | 1.24 ± 0.20 | 1.16 ± 0.21 | 2.38
Tumor | 1.10 ± 0.20 | 0.54 ± 0.10 | 0.72 ± 0.24 | - | 3.46 ± 0.66 | 1.66 ± 0.35 | 2.94 ± 1.00 | -

For complete data, see von Guggenberg et al. ( 5 )